# Microbubbles coated with anti-P-selectin antibody RB40.34

Chemical name: | Microbubbles coated with anti-P-selectin antibody RB40.34
Abbreviated name: | MB-RB40.34, MBp
Synonym:
Agent category: | Antibody
Target: | P-selectin
Target category: | Antigen
Method of detection: | Ultrasound
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=200553), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=6031196) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6403) for more information about P-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin)]

Ultrasound is the most widely used imaging modality (1) and its role in noninvasive molecular imaging with ligand-carrying microbubbles is expanding (2). Microbubbles are spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin, or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 2 to 8 μm in size. They provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They may also potentially be used for drug and gene delivery (6).

Endothelial cells are important cells in inflammatory responses (7, 8). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and secretion of other cytokines and chemokines. Leukocyte emigration from blood is dependent on rolling of leukocytes along endothelial cell surfaces and subsequent adherence to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic to leukocytes to sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space is highly orchestrated through various interactions with different adhesion molecules on endothelial cells (9).

P-selectin is found on the cell surface of endothelial cells and platelets (8, 10). It binds to glycoprotein on the cell-surface of leukocytes. IL-1 and TNFα, released from inflammatory and ischemic stimuli, stimulate P-selectin and other adhesion molecule expression on the vascular endothelial cells leading to leukocyte adhesion to the activated endothelium. P-selectin and other selectins are involved in rolling and arresting leukocytes on the endothelium. Microbubbles targeted with antibodies against P-selectin are being developed as noninvasive agents for P-selectin expression in vascular endothelial cells of inflamed and damaged tissues (11).

### Related Resource Links:

- Chapters in MICAD (P-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-selectin (http://www.ncbi.nlm.nih.gov/gene/6403)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (P-selectin (http://omim.org/entry/173610))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin)]

For targeted microbubbles, biotinylated microbubbles were first prepared by sonication of an aqueous dispersion of decafluorobutane gas, distearoylphosphatidylcholine, polyethyleneglycol (PEG)- stearate, and distearoylphosphatidylethanolamine-PEG-biotin (11). Microbubbles were combined with streptavidin, washed, and conjugated with biotinylated monoclonal antibody (RB40.34) against P-selectin (MB_p_) or isotype-control monoclonal antibody (R3-34) against α_v_ integrin (MB_iso_). Control lipid microbubbles (MB_c_) were also prepared. The microbubbles are about 3.5 ± 1.4 μm in diameter. An antibody to microbubble ratio was estimated to be 102 ± 3 x 10^3^ by flow cytometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin%20and%20in%20vitro)]

Takalkar et al. (12) reported that MB_p_ (5 x 10^6^ particles/ml) perfused through the flow chamber coated with P-selectin (109 sites/μm^2^) at a shear stress of 0.3 dyn/cm^2^ accumulated at a rate of 565 mm^-2^ min^-1^. Attachment rates increased at higher plate surface densities of P-selectin and MB_p_ detachment was reduced. Accumulation rate first increased with shear, reached a maximum stress force at ~0.6 dyn/cm^2^, and then decreased. Minimal microbubble attachment was observed on a plate that lacked P-selectin or was blocked with RB40.34. Microbubble detachment was tested by stepping up shear stress at 30-s intervals. Half-maximal detachment was reached at 34 dyn/cm^2^. Therefore, accumulation and retention of MB_p_ is possible under physiologic flow conditions and is strongly influenced by shear stress and surface density of the target receptor. Furthermore, Rychak et al. (13) demonstrated that deformed MB_p_ exhibited significantly greater attachment efficiency than spherical MB_p_ at stress forces of 0.4–1.35 dyn/cm^2^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin%20and%20rodentia)]

Lindner et al. (11) performed ultrasound assessment of inflammation with MB_p_ by intravital microscopy of the cremasteric venules of control (n = 5) and TNFα–stimulated wild-type mice (n = 5). Retention of MB_p_, MB_iso_, and MB_c_ increased (P<0.05) with TNFα treatment because of increased attachment to activated leukocytes. Extensive attachment of MB_p_ directly to the endothelium was observed in TNFα–stimulated mice, resulting in retention of MB_p_ (16 microbubbles/measurement) >3-fold (P<0.01) greater than either MB_iso_ (4 microbubbles/measurement) or MB_c_ (2 microbubbles/measurement). Enhanced retention of MB_p_ was completely abolished in TNFα–stimulated P-selectin–deficient mice. Renal ultrasound imaging of the kidneys of wild-type mice (n = 5) undergoing ischemia-reperfusion injury showed that video intensity signal was significantly higher (P<0.05) for MB_p_ (12 ± 2 U) than either MB_iso_ (6 ± 3 U) or MB_c_ (5 ± 3 U). In P-selectin-deficient mice (n = 3), the signal for MB_p_ was equivalent to that from control microbubbles.

Rychak et al. (13) demonstrated that deformed MB_p_ exhibited significantly greater attachment than spherical MB_p_ in the cremasteric venules of TNFα–treated wild-type mice (P<0.05, n = 4). There was no difference in adhesion of deformed MB_p_ and spherical MB_p_ in the cremasteric venules of TNFα–treated P-selectin–deficient mice (n = 3); rather, the adhesion measurements were 6- and 2-fold lower, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Microbubbles%20and%20P-selectin%20and%20human)]

No publication is currently available.

## NIH Support

EB02185, HL07284, HL03810, HL64381

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
8 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
9 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
10 Chen, M. and J.G. Geng, P-selectin mediates adhesion of leukocytes, platelets, and cancer cells in inflammation, thrombosis, and cancer growth and metastasis. Arch Immunol Ther Exp (Warsz), 2006
11 Lindner J.R., Song J., Christiansen J., Klibanov A.L., Xu F., Ley K. (2001). Ultrasound assessment of inflammation and renal tissue injury with microbubbles targeted to P-selectin. Circulation.
12 Takalkar A.M., Klibanov A.L., Rychak J.J., Lindner J.R., Ley K. (2004). Binding and detachment dynamics of microbubbles targeted to P-selectin under controlled shear flow. J Control Release.
13 Rychak J.J., Lindner J.R., Ley K., Klibanov A.L. (2006). Deformable gas-filled microbubbles targeted to P-selectin. J Control Release.